# [^111^In-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-10-maleimidoethylacetamide-Cys^61^]-Affibody Z_HER2:2395_

Chemical name: | [^111^In-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-10-maleimidoethylacetamide-Cys^61^]-Affibody Z_HER2:2395_
Abbreviated name: | [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | Epidermal growth factor receptor (EGFR, HER2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa), and it is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on the 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (10). Affibody molecules exhibit high binding affinity to HER2, with K_d_ values of <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A cysteine molecule was introduced at the C-terminus of Affibody molecules for site-specific coupling with the chelator 1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-10-maleimidoethylacetamide (MMA-DOTA) for ^111^In labeling. ^111^In-[MMA-DOTA-Cys^61^]-Z_HER2:2395_ (^111^In-DOTA-Z_HER2:2395_ (http://www.ncbi.nlm.nih.gov/books/NBK23711)) has been evaluated as a single-photon emission computed tomography (SPECT) agent in nude mice bearing human colon adenocarcinoma tumors (17). Altai et al. (18) prepared [^111^In-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-10-maleimidoethylacetamide-Cys^61^]-Affibody Z_HER2:2395_ ([^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_) for SPECT imaging of HER2 expression.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGF (http://www.ncbi.nlm.nih.gov/gene/1950), HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGF (http://omim.org/entry/131530), HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), HER2 imaging (http://www.clinicaltrials.gov/ct2/results?term=HER2%20and%20imaging))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20synthesis)]

Affibody Z_HER2:2395_ was reduced with dithiothreitol (30 mM) in 0.02 M ascorbic acid for 2 h at 40°C (18). The reduced Z_HER2:2395_ was incubated with MMA-NODAGA in 1:3 molar ratio in 0.2 M ammonium acetate buffer (pH, 6.5) for 1 h at 37°C. [MMA-NODAGA-Cys^61^]-Z_HER2:2395_ was isolated with high-performance liquid chromatography, with 85% of Z_HER2:2395_ conjugated and >96% purity. There was one MMA-NODAGA moiety per [MMA-NODAGA-Cys^61^]-Z_HER2:2395_ (7.5 kDa), as confirmed with mass spectroscopy_._ [MMA-NODAGA-Cys^61^]-Z_HER2:2395_ (~4 nmol) was mixed with ~30 MBq (0.81 mCi) ^111^InCl_3_ and incubated for ~30 min at 60°C, with 99% labeling yield. [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ was isolated with column chromatography. The specific activity was 7 MBq/nmol (0.19 mCi/nmol) at the end of synthesis. [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ was >99% intact after incubation with 1,000-fold excess EDTA for 60 min. The DOTA compound have similar analytical data (17).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20in%20vitro)]

Altai et al. (18) performed binding experiments with Z_HER2:2395_ with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_d_ values of Z_HER2:342_ and [MMA-NODAGA-Cys^61^]-Z_HER2:2395_ were 78 pM and 67 pM, respectively. The K_d_ value of Z_HER2:2395_ was reported to be 27 pM (17). In vitro cellular accumulation of [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ was determined to be 18% and 7% of incubation dose (ID) in human ovarian carcinoma SKOV-3 and prostate carcinoma DU-145 cells expressing HER2, respectively, for 1 h at 37°C. Co-incubation with excess unlabeled Z_HER2:342_ reduced the accumulation in both cell types to <1% ID. Internalization of [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ into DU-145 cells was 28% of the cell-associated radioactivity after 8 h of incubation. Internalization of ^111^In-[MMA-DOTA-Cys^61^]-Z_2395_-C into SKOV-3 cells was 21% of the initially bound activity at 24 h (17).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20rodentia)]

Altai et al. (18) performed ex vivo biodistribution studies with 0.03 MBq (1 μCi) [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ and [^111^In-MMA-DOTA-Cys^61^]-Z_HER2:2395_ in normal nude mice (n = 4/group) at 1, 4, and 24 h after injection. Both tracers exhibited a rapid blood clearance, with 0.45% injected dose/gram (ID/g) for the NODAGA tracer and 1.3% ID/g for the DOTA tracer in the blood at 1 h after injection. At 24 h, the blood levels were 0.03% ID/g and 0.13% ID/g for the NODAGA and DOTA tracers, respectively. In general, the NODAGA tracer exhibited lower accumulation than the DOTA tracer in most organs. The clearance of both tracers was via the kidneys, with low radioactivity in the intestines (<2% ID). The kidney accumulation levels at 4 h were 70% ID/g and 203% ID/g for [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ and [^111^In-MMA-DOTA-Cys^61^]-Z_HER2:2395_, respectively. The biodistribution was characterized by quick clearance of radioactivity from the blood and normal organs except the kidneys. No blocking studies were performed.

Altai et al. (18) performed ex vivo biodistribution studies with [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ and [^111^In-MMA-DOTA-Cys^61^]-Z_HER2:2395_ in nude mice (n = 4/group) bearing DU-145 xenografts at 4 h after injection. The tumor accumulation of radioactivity was 4.7 ± 0.8% injected dose/gram (ID/g) and 7.5 ± 1.6% ID/g, respectively. The radioactivity level in tumors was higher than in other organs and tissues (the lung, liver, spleen, bone, muscle, and intestines) except the kidneys (60% ID/g and 128% ID/g for the NODAGA and DOTA tracers, respectively). The tumor/blood ratios were 51 and 11 for the NODAGA and DOTA tracers, respectively. In general, [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ exhibited 1- to 2-fold higher tumor/tissue ratios than the DOTA tracer. Pretreatment with >3,000-fold excess Z_HER2:342_ 60 min before injection of [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ decreased tumor accumulation by >95% (P = 0.0005) at 1 h after injection. Little reduction was observed in the other organs.

SPECT gamma planar imaging scans were performed in nude mice (n = 3) bearing DU-145 tumors at 4 h after injection of 1 MBq (0.027 mCi) [^111^In-MMA-NODAGA-Cys^61^]-Z_HER2:2395_ (18). The tumors were clearly visualized along with the kidneys. The tumor/background ratio was 10, as determined with region of interest analysis. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.
18 Altai M., Perols A., Karlstrom A.E., Sandstrom M., Boschetti F., Orlova A., Tolmachev V. (2012). Preclinical evaluation of anti-HER2 Affibody molecules site-specifically labeled with (111)In using a maleimido derivative of NODAGA. Nucl Med Biol.